# Gadolinium-reconstituted high-density liproprotein-[palmitoyl-WK(palmitoyl)G(LRKLRKRLLR)_2_-NH_2_] nanoparticles

Chemical name: | Gadolinium- reconstituted high-density liproprotein-[palmitoyl-WK(palmitoyl)G(LRKLRKRLLR)_2_-NH_2_] nanoparticles
Abbreviated name: | rHDL-P2A2
Synonym:
Agent category: | Peptide
Target: | Low-density lipoprotein receptor (LDLR)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=178853), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48762938180) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=348) for more information about apolipoprotein E.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (2, 3). Gd-labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (4-6); however, these Gd complexes cannot proceed into further clinical development because of high tissue accumulation and slow excretion of toxic Gd ions. Furthermore, they are largely nonspecific.

Apolipoprotein E (apoE) is essential for the normal catabolism of triglyceride-rich lipoprotein chylomicrons (lipoprotein particles) (7). Under atherogenic conditions, deposits of lipids and extracellular matrix proteins on the endothelial cell surfaces of aortic and inflammatory cells lead to the development of atherosclerotic plaques (8), which may erode and rupture. The apoE-derived peptide A2 ((LRKLRKRLLR)_2_) is a tandem dimer derived from the low-density lipoprotein receptor (LDLR)–binding domain of apoE (9). A2 has been modified by the addition of two palmitoyl chains to form palmitoyl-WK(palmitoyl)G(LRKLRKRLLR)_2_-NH_2_ (P2A2), which can be incorporated into lipid-based nanoparticles (10). Gd-Reconstituted high-density lipoprotein nanoparticles (rHDL) have been developed for the detection of atherosclerotic plaques (11). Chen et al. (12) has incorporated a carboxyfluorescence-modified P2A2 (P2fA2) into rHDL nanoparticles (rHDL-P2A2) for imaging atherosclerotic plaques in apoE knockout mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2+synthesis)]

P2fA2, prepared with solid-phase synthesis, was incorporated into rHDL nanoparticles (12). 1,2-Dipalmitoyl-sn-glycero-3-phosphocholine (DPPC), Gd-DPTA-BSA, and rhodamine-PE were dissolved in chloroform-ethanol and then dried to a lipid film overnight. The film was dissolved in sodium cholate buffer (pH 7.5) with the addition of apoA1 and P2fA2, and the mixture was incubated for 2 h at 0–5ºC. The molar ratio of apoAI:DPPC:P2fA2:Gd-DPTA-BSA:rhodamine-PE:sodium cholate was1:113:10:25:2:200. rHDL-P2A2 nanoparticles were purified with dialysis. There were 22 and 19 Gd^3+^ ions per nanoparticle for rHDL and rHDL-P2A2, respectively. The longitudinal relaxivity (r_1_) values, measured at 60 MHz, were 11.3 and 10.5 mM^-1^s^-1^ per Gd^3+^ ion for rHDL and rHDL-P2A2, respectively. The zeta potentials of rHDL and rHDL-P2A2 were -20.3 and +15.6mV, respectively. The nanoparticles had a mean diameter of 11.6 ± 3.7 nm in aqueous solution as determined with dynamic light scattering.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2+in+vitro)]

The accumulation of rHDL and rHDL-P2A2 in macrophage J774A.1 cells was measured with fluorescent intensities and the longitudinal relaxation rates (R_1_) of the cell lysates after 24 h of incubation (12). Cell lysates from rHDL-P2A2 incubation exhibited two-fold higher fluorescent intensities than did rHDL at 0.05 nM Gd^3+^. The lysates of cells incubated with rHDL nanoparticles had an R_1_ value of 0.281 ± 0.008 s^-1^, while the cells incubated with rHDL-P2A2 nanoparticles had an R_1_ value of 0.412 ± 0.008 s^-1^. Endocytosis of both rHDL and rHDL–P2A2 into J774A.1 macrophages was confirmed with confocal images. However, rHDL–P2A2 binds to its receptor on the surface of macrophages, followed by endocytosis.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2+rodentia)]

Chen et al. (12) performed in vivo MRI imaging (9.4 T) on 6-month-old apoE^-/-^ mice that were fed a high-fat, high-cholesterol diet for 4.5 months. Animals were injected with either 50 mmol Gd/kg rHDL (n = 6 mice) or rHDL-P2A2 (n = 5 mice). Elimination of the nanoparticles was bi-exponential. The two time constants for rHDL were 125 min and 3.9 × 10^6^ min, respectively. The two time constants for rHDL-P2A2 were 39 min and 723 min. Sequential T1-weighted MRI images showed that both the rHDL and rHDL-P2A2 caused increased atherosclerotic arterial vessel wall enhancement at 24 h after injection. The mean normalized enhancement ratio of rHDL-P2A2 at 24 h after injection was 90%, whereas that of rHDL was 53% at the same time point. The signal with the rHDL was substantially reduced to 24% by 48 h. On the other hand, the enhancement ratio of rHDL-P2A2 remained high at 66% at 48 h after injection. The contrast/noise ratio of rHDL-P2A2 was 14 ± 5, significantly higher than that of rHDL (6 ± 5) at 24 h after injection. In contrast, no significant enhancement of the arterial vessel wall of wild-type mice was observed after injection of either rHDL or rHDL-P2A2. Confocal laser scanning microscopy revealed that rHDL-P2A2 co-localized primarily with intraplaque macrophages with CD68 staining. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20rHDL-A2P2+human)]

No publication is currently available.

## NIH Support

1S10 RR09145-01, 5R24 CA095823-04, R01 HL71021, R01 HL78667

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
3 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
4 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
5 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
6 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
7 Eichner J.E., Dunn S.T., Perveen G., Thompson D.M., Stewart K.E., Stroehla B.C. (2002). Apolipoprotein E polymorphism and cardiovascular disease: a HuGE review. Am J Epidemiol.
8 Libby P., Ridker P.M., Maseri A. (2002). Inflammation and atherosclerosis. Circulation.
9 Sauer I., Dunay I.R., Weisgraber K., Bienert M., Dathe M. (2005). An apolipoprotein E-derived peptide mediates uptake of sterically stabilized liposomes into brain capillary endothelial cells. Biochemistry.
10 Sauer I., Nikolenko H., Keller S., Abu Ajaj K., Bienert M., Dathe M. (2006). Dipalmitoylation of a cellular uptake-mediating apolipoprotein E-derived peptide as a promising modification for stable anchorage in liposomal drug carriers. Biochim Biophys Acta.
11 Frias J.C., Ma Y., Williams K.J., Fayad Z.A., Fisher E.A. (2006). Properties of a versatile nanoparticle platform contrast agent to image and characterize atherosclerotic plaques by magnetic resonance imaging. Nano Lett.
12 Chen W., Vucic E., Leupold E., Mulder W.J., Cormode D.P., Briley-Saebo K.C., Barazza A., Fisher E.A., Dathe M., Fayad Z.A. (2008). Incorporation of an apoE-derived lipopeptide in high-density lipoprotein MRI contrast agents for enhanced imaging of macrophages in atherosclerosis. Contrast Media Mol Imaging.